# ^11^C/^68^Ga-Labeled sel-tagged anti-epidermal growth factor receptor 2 affibody Z_HER2:342_

Chemical name: | ^11^C-Labeled sel-tagged anti-epidermal growth factor receptor 2 affibody Z_HER2:342_
Abbreviated name: | [^11^C/^68^Ga]Z_HER2:342_-ST
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor 2 (HER2)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZHER2%3A342&cmd=DetailsSearch)]

The human epidermal growth factor receptor-2 (HER2, ErbB2) modulates its activity through a tyrosine kinase signaling pathway and is involved in the development of various types of cancers (1, 2). Overexpression or amplification of the HER2 gene is known to occur in a high percentage of cancer cases (e.g., ~20% of breast cancer (BC)) and predicts a poor prognosis for the patient. Invasive methods such as biopsies in conjunction with immunohistochemistry and in situ fluorescence hybridization are often employed to assess the HER2 status of the primary and metastasized neoplastic tumors; however, because of sampling bias and tumor heterogeneity, results obtained with these procedures are not reliable (2). In the clinic, ^18^F-labeled fluorodeoxyglucose ([^18^F]-FDG) is commonly used with positron emission tomography (PET) to detect and determine the tumor burden of a patient, but this imaging agent is not able to distinguish between benign and malignant lesions, cannot differentiate tumors that overexpress HER2 from those that have a low expression or do not express the receptor, and often identifies inflammation as a false-positive neoplasm (1).

An Affibody molecule is a chain of 58 amino acids (~6.5 kDa) that contains a modified B domain of the staphylococcal protein A and can be obtained via chemical synthesis or produced in bacteria with the use of recombinant DNA technology (3). Because of their small size and high chemical and thermal stability, there is much interest to radiolabel these molecules and use them for the targeted detection and treatment of malignant tumors as discussed in detail elsewhere (3-5). Orlova et al. generated an anti-HER2 Affibody molecule (Z_HER2:342_) with a picomolar affinity for the receptor and showed that ^125^I-labeled Z_HER2:342_ can be used with gamma planar imaging to visualize xenograft SKOV-3 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-77&Template=cellBiology) cell tumors (these cells express the HER2) in mice (6). The Z_HER2:342_ Affibody has also been labeled with ^111^In or ^99m^Tc and shown to be suitable for the detection of HER2^+^ tumors with single-photon emission computed tomography (SPECT) in preclinical and clinical studies (7). Probes labeled with nuclides such as ^18^F (half-life = 109.8 min and 97% β^+^-decay) and ^11^C (half-life = 20.4 min and 100% β^+^-decay) are commonly used with PET imaging in the clinic because this technique generates images that have high spatial resolution and sensitivity and produces superior quantitative data compared with SPECT (7). Recently, ^18^F-labeled Z_HER2:342_ was shown to be suitable for the detection of HER2^+^ pulmonary metastasis with PET in mice (1). However, the only known procedure to label proteins with ^11^C is by introducing a tetrapeptide tag (sel-tag; known as Sec or U; sequence –Gly-Cys-Sec-Gly-COOH) on the C-terminus of the molecule as described by Cheng et al. (8). The properties of sel-tag are described elsewhere (9). In an effort to develop an alternate Affibody that can be used to detect HER2^+^ tumors with PET, a recombinant Z_HER2:342_ containing the sel-tag was developed (Z_HER2:342_-ST) and labeled with ^11^C/^68^Ga ([^11^C/^68^Ga]Z_HER2:342_-ST) (7). The biodistribution and use of [^11^C/^68^Ga]Z_HER2:342_-ST for the detection of HER2^+^ xenograft tumors was then investigated in severe combined immunodeficient (SCID) mice and mice bearing SKOV-3 cell tumors that have a high expression of HER2 (7).

### Related Resource Links

Anti-HER2 affibodies in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Anti-HER2+affibody+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

HER2 clinical trials (http://clinicaltrials.gov/ct2/results?term=HER2)

Other EGFR-imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad)

EGFR (human) ligands (http://www.ncbi.nlm.nih.gov/pubmed?term=Human%20EGFR%20ligands&cmd=DetailsSearch) in PubMed

Human EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Human%20EGFR) (Online Mendelian Inheritance in Man database)

Information on EGFR (human) gene (http://www.ncbi.nlm.nih.gov/protein?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=genesensor5&logdbfrom=protein)

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_005219.2?ordinalpos=17&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NG_011529.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) information regarding EGFR

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-ZHER2%3A342%20synthesis&cmd=DetailsSearch)]

Z_HER2:342_-ST was produced with recombinant techniques and covalently labeled with ^11^C as described elsewhere (7). The radiochemical yield (RCY) of the reaction was 5%–15%, and the radiochemical purity (RCP) of the final [^11^C]Z_HER2:342_-ST preparation was >97% as determined with radiographic high-performance liquid chromatography. The time taken to obtain the purified product from the end of bombardment was 40–45 min. The specific activity (SA) of the labeled Affibody was 10–30 GBq/μmol (0.37–1.17 Ci/μmol).

For use in a biodistribution study, Z_HER2:342_-ST was conjugated with 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA) and radiolabeled with ^68^Ga ([^68^Ga]Z_HER2:342_-ST-DOTA) (7). The RCY and RCP of purified [^68^Ga]Z_HER2:342_-ST-DOTA were 31% and 94%, respectively. The SA of [^68^Ga]Z_HER2:342_-ST-DOTA was reported to be 14 GBq/μmol (518 mCi/μmol).

Recombinant hexahistidine-tagged Z_HER2:342_-ST (H_6_-Z_HER2:342_-ST) and Z_EGFR:2377_-ST (H_6_-Z_EGFR:2377_-ST; Z_EGFR:2377_ is another Affibody that binds to HER2 (10) and is used as control) used in some in vitro studies were produced in and purified from Escherichia coli (7). Before use, the two Affibodies were labeled with 5-iodoacetamidofluorescine (5-IAF), a fluorescent dye, to obtain H_6_-Z_HER2:342_-ST-IAF and H_6_-Z_EGFR:2377_-ST-IAF, respectively (7).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-ZHER2%3A342-ST%20in%20vitro%20studies&cmd=DetailsSearch)]

Instant thin-layer chromatographic analysis of [^68^Ga]Z_HER2:342_-ST-DOTA incubated with either 500-fold molar excess ethylenediaminetetraacetic acid or in water alone at room temperature for 60 min showed that 90%–95% of the radioactivity remained associated with the Affibody (7). When [^68^Ga]Z_HER2:342_-ST-DOTA was incubated with murine plasma for 1 h at 37°C, no transchelation of the radionuclide to serum proteins was observed, as determined with sodium dodecyl sulfate polyacrylamide gel electrophoresis (7). These studies indicated that [^68^Ga]Z_HER2:342_-ST-DOTA remained stable under these in vitro conditions.

Fluorescence-activated cell-sorting analysis of SKOV-3 cells, MDA-MB-453 cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-131&Template=cellBiology) (have high expression of HER2), and A431 cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2592&Template=cellBiology) (exhibit very low expression of HER2) exposed to H_6_-Z_HER2:342_-ST-IAF or H_6_-Z_EGFR:2377_-ST-IAF showed that the two Affibodies bound only to the SKOV-3 cells and the MDA-MB-453 cells (7). When the SKOV-3 cells and MDA-MB-453 cells were blocked with 10-fold excess of non-radiolabeled Affibody (dose not mentioned), a significant reduction in the binding of both H_6_-Z_HER2:342_-ST-IAF and H_6_-Z_EGFR:2377_-ST-IAF to the two cell lines was observed. This study indicated that the sel-tag or the labeling of the two Affibodies with 5-IAF did not affect the HER2-binding specificity of the molecules (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-ZHER2%3A342-ST%20rodentia&cmd=DetailsSearch)]

The biodistribution of ^11^C- and ^68^Ga-labeled Z_HER2:342_-ST was compared in two SCID mice as described by Wallberg et al. (7). The animals were administered 3–4 MBq (111–148 μCi; 2.7 nmol) [^11^C]Z_HER2:342_-ST through the tail vein, and whole-body PET images of the mice were acquired for up to 1 h postinjection (p.i.). After >3 h (to allow complete decay of ^11^C; >10 half-lives), the same animals were injected with 7–8 MBq (259–296 μCi; 0.4 nmol) [^68^Ga]Z_HER2:342_-ST-DOTA through the same route as mentioned above, and whole-body PET images were obtained from the rodents for up to 1 h p.i. From the images it was determined that the circulation half-lives of [^11^C]Z_HER2:342_-ST and [^68^Ga]Z_HER2:342_-ST-DOTA were 2 h and 6 h, respectively. At 1 h p.i., the amount of radioactivity in the blood was 3.9% injected dose per gram tissue (% ID/g) and 4.9% ID/g with the ^11^C- and ^68^Ga-labeled Affibodies, respectively. The amount of ^68^Ga in the kidneys was reported to be five-fold higher than that of ^11^C at 1 h p.i., indicating that ^68^Ga was probably reabsorbed in the proximal tubules of the organs and trapped within the organ (7).

The tumor targeting ability of [^11^C]Z_HER2:342_-ST was investigated in mice bearing SKOV-3 cell xenograft tumors (7). For this study, animals bearing A431 cell tumors were used as controls. The animals (n = 8 mice) were injected with 4–8 MBq (148–196 μCi; 0.8–3.4 nmol) of the labeled Affibody through the tail vein, and whole-body imaging was performed on the rodents for the next 1 h. To determine the tumor-targeting specificity of [^11^C]Z_HER2:342_-ST, the same animals were given a subcutaneous or intravenous injection of 33 nmol of the non-radioactive Affibody, injected with [^11^C]Z_HER2:342_-ST 1 h later, and imaged for 1 h. Time-activity curves of the unblocked animals showed that the maximum uptake of radioactivity in the tumors was 9.9 ± 1.8% ID/g at 32.5 min p.i. In the blocked animals, the maximum uptake of radioactivity in the tumors was 5.0 ± 1.3% ID/g at 30 min p.i. (P = 0.002). In general, the biodistribution of radioactivity in the unblocked and blocked rodents was similar to that observed in the SCID mice (described above). The A431 cell tumors showed a significantly lower uptake of the label compared the SKOV-3 cell lesions (P = 0.0001). This study demonstrated that [^11^C]Z_HER2:342_-ST had a binding specificity for the HER2^+^ tumors in the animals (7).

From these studies, the investigators concluded that Affibody molecules can be tagged with the sel tetrapeptide, radiolabeled with ^11^C, and used as a targeted imaging probe in rodents (7).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-ZHER2%3A342-ST%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-ZHER2%3A342-ST%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-ZHER2%3A342-ST%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Kramer-Marek G., Bernardo M., Kiesewetter D.O., Bagci U., Kuban M., Omer A., Zielinski R., Seidel J., Choyke P., Capala J. (2012). PET of HER2-Positive Pulmonary Metastases with 18F-ZHER2:342 Affibody in a Murine Model of Breast Cancer: Comparison with 18F-FDG. J Nucl Med.
2 Kramer-Marek G., Gijsen M., Kiesewetter D.O., Bennett R., Roxanis I., Zielinski R., Kong A., Capala J. (2012). Potential of PET to predict the response to trastuzumab treatment in an ErbB2-positive human xenograft tumor model. J Nucl Med.
3 Feldwisch J., Tolmachev V., Lendel C., Herne N., Sjoberg A., Larsson B., Rosik D., Lindqvist E., Fant G., Hoiden-Guthenberg I., Galli J., Jonasson P., Abrahmsen L. (2010). Design of an optimized scaffold for affibody molecules. J Mol Biol.
4 Lofblom J., Feldwisch J., Tolmachev V., Carlsson J., Stahl S., Frejd F.Y. (2010). Affibody molecules: engineered proteins for therapeutic, diagnostic and biotechnological applications. FEBS Lett.
5 Tolmachev V., Orlova A. (2010). Influence of labelling methods on biodistribution and imaging properties of radiolabelled peptides for visualisation of molecular therapeutic targets. Curr Med Chem.
6 Orlova A., Magnusson M., Eriksson T.L., Nilsson M., Larsson B., Hoiden-Guthenberg I., Widstrom C., Carlsson J., Tolmachev V., Stahl S., Nilsson F.Y. (2006). Tumor imaging using a picomolar affinity HER2 binding affibody molecule. Cancer Res.
7 Wallberg H., Grafstrom J., Cheng Q., Lu L., Martinsson Ahlzen H.S., Samen E., Thorell J.O., Johansson K., Dunas F., Olofsson M.H., Stone-Elander S., Arner E.S., Stahl S. (2012). HER2-Positive Tumors Imaged Within 1 Hour Using a Site-Specifically 11C-Labeled Sel-Tagged Affibody Molecule. J Nucl Med.
8 Cheng Q., Lu L., Grafstrom J., Olofsson M.H., Thorell J.O., Samen E., Johansson K., Ahlzen H.S., Stone-Elander S., Linder S., Arner E.S. (2012). Combining [(11)C]-AnxA5 PET Imaging with Serum Biomarkers for Improved Detection in Live Mice of Modest Cell Death in Human Solid Tumor Xenografts. PLoS One.
9 Cheng Q., Stone-Elander S., Arner E.S. (2006). Tagging recombinant proteins with a Sel-tag for purification, labeling with electrophilic compounds or radiolabeling with 11C. Nat Protoc.
10 Tolmachev V., Rosik D., Wallberg H., Sjoberg A., Sandstrom M., Hansson M., Wennborg A., Orlova A. (2010). Imaging of EGFR expression in murine xenografts using site-specifically labelled anti-EGFR 111In-DOTA-Z EGFR:2377 Affibody molecule: aspect of the injected tracer amount. Eur J Nucl Med Mol Imaging.